# ^99m^Tc-Ubiquicidin_29-41_

Chemical name: | ^99m^Tc-Ubiquicidin_29-41_
Abbreviated name: | ^99m^Tc-UBI_29-41_
Synonym:
Agent Category: | Peptide
Target: | Microbial cell membrane
Target Category: | Membrane binding
Method of detection: | SPECT, planar gamma
Source of signal: | ^99m^Tc
Activation: | Not required
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Structure of ^99m^Tc-UBI_29-41_ as proposed by Meléndez-Alafort et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+Human)]

It has been reported that almost 85% of critically ill patients in hospitals have fever but show no apparent signs of infection (2, 3). Prolonged febrile episodes are often fatal, so the detection of infection at an early stage is important in patient management to achieve a favorable treatment outcome. Radiological (x-ray computed tomography) and imaging (magnetic resonance imaging) techniques are often not suitable for the early detection of infection because such techniques are focused on specific body parts and provide information only if morphological changes have occurred in the applied areas (4, 5). In contrast, scintigraphy can scan the entire body and easily detect and distinguish between an infection and inflammation because it relies on functional, morphologically invisible, changes in the tissue (6). A variety of radiolabeled compounds, including ^67^Ga-citrate, ^111^In- or ^99m^Tc-labeled human immunoglobulins, monoclonal antibodies that interact with specific receptors on the infiltrating leukocytes, and peptides have been evaluated for the detection of infections (5). However, because they accumulate in both infected and inflamed areas of the body, these radiopharmaceuticals are non-specific and can not distinguish between infection and inflammation (4).

In an effort to identify and develop radioactive compounds that are specific for the detection of infections, various investigators have evaluated the use of antimicrobial peptides that are found naturally in most multicellular organisms (5, 7). Such peptides bind specifically to microbes, presumably through cationic domains that interact with anionic regions of the microbial membrane (8), and were shown to distinguish infected from inflamed tissue (9-11). Hiemstra et al. identified, isolated, and characterized a unique 6.7-kDa protein, ubiquicidin (UBI), from the cytosolic fraction of murine macrophages and showed that it had antimicrobial activity against Lysteria monocytogenes and Salmonella typhimurium (12). A 13mer peptide derived from UBI, designated as UBI_29-41_, is being evaluated for antimicrobial activity and ability to detect infections in preclinical and clinical settings (9, 10, 13). The peptide was labeled with ^99m^Tc to obtain ^99m^Tc-UBI_29-41_ and it has been used in the various studies.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+synthesis)]

The synthetic 13mer UBI_29-41_ peptide, based on the α helical domain of UBI, was used in most studies presented in this chapter. It was synthesized by using solid-phase strategies with an automated process (14). Using the same process, a scrambled version of the peptide was also synthesized and used as a control (11).

To label the peptide, a stock solution of the peptide was added to an aseptic mixture of stannous chloride and sodium pyrophosphate in saline, and a solution of potassium borohydrate in sodium hydroxide (NaOH) was added to the mixture. A solution of freshly eluted ^99m^Tc-sodium pertechnetate (200 MBq/ml (5.40 mCi/ml)) was added to the mixture and gently stirred for at least 10 min at room temperature. The solution was then ready for use. The preparation was analyzed with high-performance liquid chromatography (HPLC), and recovery of the radioactivity was 83 ± 13% (n = 10) with a labeled peptide yield of 98 ± 0.2% as determined by instant thin-layer chromatography (ITLC); Rf values for the ITLC were not provided by the investigators. To determine the presence of any ^99m^Tc-colloids in the preparations, the labeled peptides were diluted in 0.1% (v/v) acetic acid (HAc) and applied to a Sep-Pak Light C_18_ cartridge. The column was washed with 0.1% (v/v) HAc until no detectable amount of radioactivity was recovered. The column was then washed with methanol and the trapped radioactivity was recovered. Less than 5% of total radioactivity in the samples was determined to be from colloids.

A lyophilized labeling kit for UBI_29-41_ was developed and used to perform some studies, including those on humans (13, 15). The kit contained 400 µg of the peptide dissolved in 0.01 mol/L acetic acid along with stannous ions (concentration not available) from a standard pyrophosphate kit, and 0.7 mg/mL sodium borohydrate in 0.1 N NaOH; pH of the mixture was maintained between 6 and 7. The preparation was freeze-dried and sealed under vacuum (15). To label the peptide, 200 MBq/ml (5.40 mCi/ml) of freshly eluted sodium pertechnetate (^99m^Tc ) was added to the vial. The mixture was incubated at room temperature for 10–15 min and 0.9% saline was added to the vial to obtain a final volume of 2.0 ml. The kit was stored at room temperature and used within 6 h of reconstitution. For quality control of the kit preparation, paper chromatography was used to determine the free activity in the reconstituted kit, ITLC was used to determine the hydrolyzed activity, and HPLC was used to determine sample purity. Although sample purity was not reported by the investigators, pertechnetate in the preparation was reported to be <1% and, in general, labeling efficiency for the labeled peptide was determined to be >95%. These values did not change for up to 6 h after the labeling reaction.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+in+vitro+studies)]

High thermodynamic stability, selectivity, and stereospecificity of ^99m^Tc-UBI_29-41_ are believed to contribute to the in vitro bacterial binding specificity and its accumulation at infection sites in humans (16). The binding of ^99m^Tc-UBI_29-41_ to human cell lines was investigated using ACHN (of renal adenocarcinoma origin) and LS174T (of colon cancer origin) cells. Binding of the labeled peptide to the human cells was also compared to binding to Staphylococcus aureus bacterial cells (17). It was reported that 87% of the labeled peptide bound to the bacteria, but <4% of the label bound to the human cells under the study conditions. The investigators proposed that the arginine-rich ^99m^Tc-UBI_29-41_ peptide binds primarily to bacterial cells because the eukaryotic cells have a specific receptor that is not found on mammalian cell membranes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+rodentia)]

In a study with mice, Welling et al. showed that ^99m^Tc-UBI_29-41_ accumulated in tissues infected with either gram-positive or gram-negative bacteria or even Candida albicans (18). Welling et al. also observed that ^99m^Tc-UBI_29-41_ had a significantly lower (P < 0.01) accumulation in sterile inflamed tissue. For comparison, ^99m^Tc-labeled ciprofloxican was also injected into infected animals and it was observed not to distinguish between infections and sterile inflammation. ^99m^Tc-UBI_29-41_ was also shown to be a superior agent for the detection of infection compared to ^67^Ga-labeled citrate because ^99m^Tc-UBI_29-41_ had an average infection/inflammation ratio of 2.08 ± 0.49 compared to a ratio of 1.14 ± 0.45 obtained with ^67^Ga-citrate (17). Using mice and rats, Nibbering et al. demonstrated that ^99m^Tc-UBI_29-41_ could be used to monitor the efficacy of antibacterial agents such as cloxacillin, erythromycin, and hLF, an antimicrobial peptide derived from human lactoferrin (19). The investigators showed there was a good correlation between the accumulation of ^99m^Tc-UBI_29-41_ at the site of infection and the number of viable S. aureus cells at the infected site. A decreased accumulation of ^99m^Tc-UBI_29-41_ was observed with a decreasing number of bacteria when the animals were treated with increasing doses of the various antimicrobial agents. In competition studies unlabeled UBI_29-41_, when injected into the mice prior to treatment with ^99m^Tc-UBI_29-41_, was shown to significantly (P < 0.05) reduce the accumulation of label at the site of infection (11). Investigators from the same laboratory also demonstrated that ^99m^Tc-labeled 6-hydrazinonicotinic (HYNIC) and diaminedithiol (N_2_S_2_) derivatives of UBI_29-41_ were equally effective for the detection of intramuscular bacterial infections in mice as ^99m^Tc-UBI_29-41_ was (20). From this study the investigators concluded that the N_2_S_2_ derivative of UBI_29-41_ could not be used for the detection of infections in the abdomen because it was cleared from the body through the liver and the intestines. In contrast, the other two tracers were eliminated from circulation primarily through the urinary system.

### Other Non-Primate Mammals

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+Other+Non-Primate+Mammals)

A high target/non-target (T/NT) ratio (>5) was observed when ^99m^Tc-UBI_29-41_ was administered to rabbits infected with Klebsiella pneumoniae (21). No accumulation of ^99m^Tc-UBI_29-41_ was observed in the thighs of rabbits previously injected with lipopolysaccharide, which indicated that the labeled peptide had a specificity for infected sites in the animals. On the basis of these observations, the investigators suggested that ^99m^Tc-UBI_29-41_ could be used for the detection of infections in humans. Using infected rabbits injected with ^99m^Tc-UBI_29-41_ generated from a freeze-dried kit, Akhtar et al. demonstrated that the labeled peptide showed less accumulation at sites infected with Escherichia coli than S. aureus (15). They reported that the optimal time for imaging a bacterial infection in the animals was 60 min after injection of the radiochemical. They also suggested that the lower signal observed with E. coli compared to S. aureus could be either because of a lower virulence of the bacterial strain used or to the result of a reduced affinity of the peptide for the bacterial membranes.

In another study, Sarda-Mantel et al. demonstrated that ^99m^Tc-UBI_29-41_ could be used to differentiate between acute prosthetic joint infections and chronic sterile joint inflammation in rabbits (10).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+Non-Human+Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc-UBI+29-41+Human)]

Meléndez-Alafort et al. evaluated the use of ^99m^Tc-UBI_29-41_ as an infection imaging agent in humans. Whole-body images were obtained for 6 children suspected of having bone infection at various time points after the administration of ^99m^Tc-UBI_29-41_ (22). The absorbed dose of radioactivity was evaluated in the heart, liver, kidneys, and the bladder at each time point for all patients treated under the protocol. For controls, images were also obtained from all the patients after the administration of ^67^Ga-citrate. ^99m^Tc-UBI_29-41_ was reported to have a fast blood clearance with a mean residence time of 0.52 h, and ~85% of the activity was cleared through the bladder within 24 h of administration. Minimal accumulation was observed in the non-target tissue and the average T/NT ratio was 2.18 ± 0.74 at 2 h for the infected tissue. Images obtained with ^99m^Tc-UBI_29-41_ were in agreement with those obtained with ^67^Ga-citrate. From this study it was concluded ^99m^Tc-UBI_29-41_ could be used for the detection of infections in humans (22).

In a similar study in adults, a gradual decline in radioactivity was observed in the kidneys and the liver from 30 to 120 min after administration of ^99m^Tc-UBI_29-41_, and during the same period the label accumulated gradually in the bladder (13). Of the 18 subjects who participated in the trial, 14 were positive for infection as determined with the use of ^99m^Tc-UBI_29-41_. These observations were confirmed by bacterial cultures; one positive case was determined to be a false positive because no bacterial growth was obtained from that specimen. The investigators concluded that ^99m^Tc-UBI_29-41_ is a promising agent for the imaging of infection with an optimal visualization at 30 min after administration of the radiochemical.

## References

1 Melendez-Alafort L., Ramirez Fde M., Ferro-Flores G., Arteaga de Murphy C., Pedraza-Lopez M., Hnatowich D.J. (2003). Lys and Arg in UBI: a specific site for a stable Tc-99m complex?. Nucl Med Biol.
2 Circiumaru B., Baldock G., Cohen J. (1999). A prospective study of fever in the intensive care unit. Intensive Care Med.
3 Rizoli S.B., Marshall J.C. (2002). Saturday night fever: finding and controlling the source of sepsis in critical illness. Lancet Infect Dis.
4 Becker W., Meller J. (2001). The role of nuclear medicine in infection and inflammation. Lancet Infect Dis.
5 Lupetti A., Welling M.M., Pauwels E.K., Nibbering P.H. (2003). Radiolabelled antimicrobial peptides for infection detection. Lancet Infect Dis.
6 Rennen H.J., Boerman O.C., Oyen W.J., Corstens F.H. (2001). Imaging infection/inflammation in the new millennium. Eur J Nucl Med.
7 Martin E., Ganz T., Lehrer R.I. (1995). Defensins and other endogenous peptide antibiotics of vertebrates. J Leukoc Biol.
8 Lupetti A., Nibbering P.H., Welling M.M., Pauwels E.K. (2003). Radiopharmaceuticals: new antimicrobial agents. Trends Biotechnol.
9 Lupetti A., Welling M.M., Mazzi U., Nibbering P.H., Pauwels E.K. (2002). Technetium-99m labelled fluconazole and antimicrobial peptides for imaging of Candida albicans and Aspergillus fumigatus infections. Eur J Nucl Med Mol Imaging.
10. Sarda-Mantel, L., A. Saleh-Mghir, M.M. Welling, A. Meulemans, J.M. Vrigneaud, O. Raguin, F. Hervatin, G. Martet, F. Chau, R. Lebtahi, and D. Le Guludec, Evaluation of (99m)Tc-UBI 29-41 scintigraphy for specific detection of experimental Staphylococcus aureus prosthetic joint infections. Eur J Nucl Med Mol Imaging, 2007.
11 Welling M.M., Mongera S., Lupetti A., Balter H.S., Bonetto V., Mazzi U., Pauwels E.K., Nibbering P.H. (2002). Radiochemical and biological characteristics of 99mTc-UBI 29-41 for imaging of bacterial infections. Nucl Med Biol.
12 Hiemstra P.S., van den Barselaar M.T., Roest M., Nibbering P.H., van Furth R. (1999). Ubiquicidin, a novel murine microbicidal protein present in the cytosolic fraction of macrophages. J Leukoc Biol.
13 Akhtar M.S., Qaisar A., Irfanullah J., Iqbal J., Khan B., Jehangir M., Nadeem M.A., Khan M.A., Afzal M.S., Ul-Haq I., Imran M.B. (2005). Antimicrobial peptide 99mTc-ubiquicidin 29-41 as human infection-imaging agent: clinical trial. J Nucl Med.
14 de Koster H.S., Amons R., Benckhuijsen W.E., Feijlbrief M., Schellekens G.A., Drijfhout J.W. (1995). The use of dedicated peptide libraries permits the discovery of high affinity binding peptides. J Immunol Methods.
15 Akhtar M.S., Iqbal J., Khan M.A., Irfanullah J., Jehangir M., Khan B., Ul-Haq I., Muhammad G., Nadeem M.A., Afzal M.S., Imran M.B. (2004). 99mTc-labeled antimicrobial peptide ubiquicidin (29-41) accumulates less in Escherichia coli infection than in Staphlococcus aureus infection. J Nucl Med.
16 Ferro-Flores G., de Maria Ramirez F., Melendez-Alafort L., de Murphy C.A., Pedraza-Lopez M. (2004). Molecular recognition and stability of 99mTc-UBI 29-41 based on experimental and semiempirical results. Appl Radiat Isot.
17 Ferro-Flores G., Arteaga de Murphy C., Pedraza-Lopez M., Melendez-Alafort L., Zhang Y.M., Rusckowski M., Hnatowich D.J. (2003). In vitro and in vivo assessment of 99mTc-UBI specificity for bacteria. Nucl Med Biol.
18 Welling M.M., Lupetti A., Balter H.S., Lanzzeri S., Souto B., Rey A.M., Savio E.O., Paulusma-Annema A., Pauwels E.K., Nibbering P.H. (2001). 99mTc-labeled antimicrobial peptides for detection of bacterial and Candida albicans infections. J Nucl Med.
19 Nibbering P.H., Welling M.M., Paulusma-Annema A., Brouwer C.P., Lupetti A., Pauwels E.K. (2004). 99mTc-Labeled UBI 29-41 peptide for monitoring the efficacy of antibacterial agents in mice infected with Staphylococcus aureus. J Nucl Med.
20 Welling M.M., Visentin R., Feitsma H.I., Lupetti A., Pauwels E.K., Nibbering P.H. (2004). Infection detection in mice using 99mTc-labeled HYNIC and N2S2 chelate conjugated to the antimicrobial peptide UBI 29-41. Nucl Med Biol.
21 Welling M.M., Paulusma-Annema A., Balter H.S., Pauwels E.K., Nibbering P.H. (2000). Technetium-99m labelled antimicrobial peptides discriminate between bacterial infections and sterile inflammations. Eur J Nucl Med.
22 Melendez-Alafort L., Rodriguez-Cortes J., Ferro-Flores G., Arteaga De Murphy C., Herrera-Rodriguez R., Mitsoura E., Martinez-Duncker C. (2004). Biokinetics of (99m)Tc-UBI 29-41 in humans. Nucl Med Biol.